# ^111^In-Diethylenetriaminepentaacetic acid-2-(p-isothiocyanatobenzyl)-6-methyl-B3 monoclonal antibody

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-2-(p-isothiocyanatobenzyl)-6-methyl-B3 monoclonal antibody
Abbreviated name: | ^111^In-DTPA-1B4M-B3, ^111^In-DTPA-MX-B3
Synonym:
Agent category: | Antibody
Target: | Lewis antigens
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20B3)]

Blood group antigens Lewis^y^ and Lewis^x^ are glycoproteins found to be expressed in a number of adenocarcinomas of diverse origin (1-4). The monoclonal antibody (mAb) B3 was directed against a carbohydrate epitope found on Lewis^y^ and Lewis^x^ antigens (5). ^111^In-Diethylenetriaminepentaacetic acid-2-(p-isothiocyanatobenzyl)-6-methyl-B3 mAb (^111^In-DTPA-1B4M-B3) has been studied for use in imaging Lewis^y^ and Lewis^x^ antigen expression in nude mice bearing human cancer xenografts (6) and in cancer patients (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20B3+synthesis)]

Camera et al. (6) reported the radiolabeling of mAb B3 for preclinical studies. DTPA-1B4M-B3 (~6.6 nmol) was mixed with 37 MBq (1 mCi) ^111^InCl_3_ in acetate buffer (pH 5.5). The mixture was incubated for 30 min at room temperature. ^111^In-DTPA-1B4M-B3 was purified with high-performance liquid chromatography with >98% radiochemical purity. The labeling efficiency for ^111^In was 68% with a specific activity of ~3.8 MBq/nmol (0.1 mCi/nmol). The number of DTPA molecules per antibody was not reported. Pai-Scherf et al. (7) prepared ^111^In-DTPA-1B4M-B3 for clinical studies with a specific activity of 41 ± 10 MBq/nmol (1.11 ± 0.27 mCi/nmol) and >99% purity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20B3+in+vitro)]

Radioimmunoreactivity of ^111^In-DTPA-1B4M-B3 for Lewis^y^ and Lewis^x^ antigens was determined by measuring ^111^In-DTPA-1B4M-B3 binding to A431 cancer cells, which was found to be >70% at infinite antigen excess (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20B3+rodentia)]

Camera et al. (6) performed biodistribution studies with ^111^In-DTPA-1B4M-B3 in nude mice bearing A431 xenografts. The percentage of injected dose per gram (% ID/g) was determined in various tissues at 24, 48, 72, 120, and 168 h after injection. Peak tumor accumulation occurred at 72 h with 25.4% ID/g. The organ with the highest accumulation was the intestine (8% ID/g), followed by the kidney, lung, liver, and spleen (4–6% ID/g) at 72 h. The tumor/blood ratios were 1.9, 3.5, and 5.3 at 24, 72, and 168 h, respectively. Single-photon emission computed tomography scintigraphic imaging showed equal amounts of radioactivity at 24 h after injection in the tumor and in the abdomen area. However, the tumor was clearly visualized by 72 h with the highest tumor/background ratio at 144 h as the radioactivity of the abdomen area decreased. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20B3+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium%20B3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+B3+human)]

Pai-Scherf et al. (7) studied patients (n = 26) with advanced epithelial tumors that express the Lewis^Y^ antigen. All patients received 185 MBq (5 mCi) ^111^In-DTPA-1B4M-B3 for imaging. Tumors were identified in 20 of 26 patients with scintillation camera images. The blood clearance pattern exhibited a half-life of 75 ± 40 h during the elimination phase (β). The mean doses to the liver and spleen were 5.2 ± 1.2 and 6.0 ± 2.3 mGy/MBq (19.4 ± 4.5 and 22.2 ± 8.6 rad/mCi), respectively. The marrow dose estimated from the biopsy was 2.2 ± 0.8 mGy/MBq (8.3 ± 3.1 rad/mCi). The mean dose to the tumor was 6.8 ± 4.9 mGy/MBq (25.1 ± 18.3 rad/mCi).

## NIH support

Intramural Research Program

## References

1 Cordon-Cardo C., Lloyd K.O., Sakamoto J., McGroarty M.E., Old L.J., Melamed M.R. (1986). Immunohistologic expression of blood-group antigens in normal human gastrointestinal tract and colonic carcinoma. Int J Cancer.
2 Cordon-Cardo C., Reuter V.E., Finstad C.L., Sheinfeld J., Lloyd K.O., Fair W.R., Melamed M.R. (1989). Blood group-related antigens in human kidney: modulation of Lewis determinants in renal cell carcinoma. Cancer Res.
3 Kanai T., Hirohashi S., Upton M.P., Ino Y., Shimosato Y. (1987). Expression of Lewis blood group antigens in cancerous and non-cancerous liver. Jpn J Cancer Res.
4 Motzer R.J., Reuter V.E., Cordon-Cardo C., Bosl G.J. (1988). Blood group-related antigens in human germ cell tumors. Cancer Res.
5 Pastan I., Lovelace E.T., Gallo M.G., Rutherford A.V., Magnani J.L., Willingham M.C. (1991). Characterization of monoclonal antibodies B1 and B3 that react with mucinous adenocarcinomas. Cancer Res.
6 Camera L., Kinuya S., Pai L.H., Garmestani K., Brechbiel M.W., Gansow O.A., Paik C.H., Pastan I., Carrasquillo J.A. (1993). Preclinical evaluation of 111In-labeled B3 monoclonal antibody: biodistribution and imaging studies in nude mice bearing human epidermoid carcinoma xenografts. Cancer Res.
7 Pai-Scherf L.H., Carrasquillo J.A., Paik C., Gansow O., Whatley M., Pearson D., Webber K., Hamilton M., Allegra C., Brechbiel M., Willingham M.C., Pastan I. (2000). Imaging and phase I study of 111In- and 90Y-labeled anti-LewisY monoclonal antibody B3. Clin Cancer Res.